# Ferumoxides

Chemical name: | Ferumoxides
Abbreviated name: | SSPIO
Synonym: | Dextran-coated superparamagnetic iron oxide, AMI-25, SHU 555A
Agent Category: | Superparamagnetic Iron Oxide
Target: | Reticuloendothelial system
Target Category: | Internalized by phagocytes
Method of detection: | Magnetic Resonance imaging (MRI)
Source of signal\contrast: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxides%22%5BSubstance%20Name%5D)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules. Water comprises about 80% of most soft tissues. The contrast of proton MRI depends mainly on the density of nuclear (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most of the contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T-2* is the spin-spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1).

Superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^) in the general formula of Fe_2_^3+^OFe^2+^O. The iron oxides particles are coated with a layer of dextran or other polysaccharide. These particles have a large combined magnetic moments or spins which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in MRI though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into the reticuloendothelial system (RES) is by endocytosis or phagocytosis. SPIO particles are taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. A variety of cells can also be labeled with these particles for cell trafficking and tumor-specific imaging studies. SPIO agents are classified by their sizes with coating material (about 20 nm to 3,500 nm in diameters) as large SPIO agents (Ferumoxsil or AMI-121, Ferucarbotran, OMP), standard SPIO (SSPIO) agents (Ferumoxides or AMI-25, SHU 555A), ultrasmall SPIO (USPIO) agents (Ferumoxtran or AMI-277, NC100150) and monocrystalline iron oxide nanoparticles (MION) agents (1).

Ferumoxides are composed of iron particles of about 5 nm, and the hydrodynamic diameter is about 80-150 nm. The crystals are covered with a layer of dextran. Ferumoxides are classified as SSPIO. Ferumoxides have been tested in clinical trials as negative contrast agents that decrease signal on T2 images. Ferumoxides have been used in liver, spleen, and myocardial perfusion MR imaging (1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxides%22%5BSubstance%20Name%5D%20AND%20synthesis)]

SPIO agents are produced by controlling the precipitation of iron oxide in an aqueous solution of ferric salt, ferrous salt, and coating material by addition of an alkaline solution while active stirring or sonication is applied. The desired SPIO size of the agent is isolated and purified by differential column chromatography, centrifugation, and dialysis. Electron microscopy, X-ray diffraction and laser light scattering are used to measure median diameter of the nanoparticles. Relaxivities are measured by NMR spectroscopy (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxides%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

It was shown that the uptake of SPIO by human monocytes was dependent on size, concentration, and time. SSPIO uptake was higher than USPIO uptake as measured by iron content and T2* relaxivity. The uptakes of both were directly proportional to concentration and time. The surface property of SPIO is also an important factor (2) (3).

In the presence of polyinosinic acid or fucoidan (specific ligands of scavenger receptors SR-A types I and II), the endocytosis of AMI-25 by mouse peritoneal macrophages was inhibited in a dose-dependent manner. Without competitors, uptake of AMI-25 by mouse peritoneal macrophages ranged between 3% and 8%. On human activated monocyte THP-1 cell assay, AMI-25 showed a higher macrophage uptake (between 1.1 and 3%) compared with USPIO (between 0.03 and 0.12%). This difference is attributed to the larger size of AMI-25 nanoparticles (2).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxides%22%5BSubstance%20Name%5D%20AND%20%22rodentia%22%5BMeSH%20Terms%5D)]

The blood half-life of USPIO (the hydrodynamic diameter is about 11 nm) in rats was 81 min, considerably longer than that of larger SPIO preparations, such as AMI-25 (6 min). AMI-25 showed a rapid clearance by the liver and spleen, with no detectable uptake in the lymph nodes. Peak concentrations of iron were found in the liver after 2 h and in the spleen after 4 h. Iron was cleared slowly from the liver and spleen with a half-life of 3 and 4 days, respectively (4). Myocardial T2-weighted signal decreased in rat hearts after AMI-25 infusion in normal rats. The intensity remained constant in the rat heart transplants during coronary occlusion, both before and after the infusion of AMI-25 and decreased further upon reperfusion. Therefore, AMI-25 is able to identify normal, ischemic, and reperfused myocardium (5).

Atherosclerotic plaques in cytokine-treated mice contained more iron-positive macrophages per cross section than did those in sham-treated control mice. Iron-laden macrophages were present either in subendothelial plaque surfaces or in thin layers overlying the internal elastic lamina, often at the edges of atherosclerotic plaques. No iron deposition was seen in aortas of the wild-type, non-atherosclerotic control mice. Immunocytochemistry showed mostly macrophages and few T lymphocytes in atherosclerotic plaques of cytokine-treated mice (6).

Bos et al. (7) were able to track intravascularly injected, ferumoxide-labeled mesenchymal stem cells in rat kidney and liver using in vivo MRI T2* measurements. The labeled cells were able to differentiate into adipocytes and osteocytes in cultures. The cells were detected up to 7 days in the kidney and 12 days in the liver. Immunohistochemical analysis results confirmed these mesenchymal stem cells in renal glomeruli and hepatic sinusoids. Additional studies are needed to evaluate stem cell differentiation and to assess resultant cellular function in vivo in the target organs.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxides%22%5BSubstance%20Name%5D%20AND%20%22animals%22%5BMeSH%5D%20NOT%20%22rodentia%22%5BMeSH%5D%20NOT%20%22primates%22%5BMeSH%5D)]

Rabbits were injected with SPIO nanoparticles to evaluate liver localization and magnetic resonance appearance. Small (30 nm), standard (300 nm) and large SPIO particles (3,500 nm) reduced the T2 of liver by 50%, 40% and 15%, respectively, and the T2 of spleen by 60%, 65%, and 25%, respectively, at 1 mg Fe/kg intravenous injection. Both small and standard SPIO nanoparticles decreased the T1 of spleen by 35%, with no effect on liver T1. Magnetic resonance imaging showed decreased signal intensity ratios by 80% and 60% for small and standard SPIO nanoparticles, respectively (8).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxides%22%5BSubstance%20Name%5D%20AND%20%22Primates%22%5BMeSH%20Terms%5D%20NOT%20%22rodentia%22%5BMeSH%5D%20NOT%20%22humans%22%5BMeSH%5D)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxides%22%5BSubstance%20Name%5D%20AND%20%22humans%22%5BMeSH%20Terms%5D)]

Ferumoxides-enhanced MR imaging significantly increases tumor/liver contrast and improves tumor lesion recognition on T2-weighted images (9). A 95% sensitivity for metastatic tumor detection was reported by using ferumoxides-enhanced MR imaging (10). In a large multi-center trial, additional liver tumors were identified on 27% of ferumoxides-enhanced images compared with non-enhanced images (11). The major potential applications for ferumoxides are as (a) an intravenous contrast agent for the liver [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxides%22%5BSubstance%20Name%5D%20AND%20%22humans%22%5BMeSH%20Terms%5D%20AND%20%22liver%22%5BMeSH%20Terms%5D)], (b) a spleen contrast agent [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxides%22%5BSubstance%20Name%5D%20AND%20%22humans%22%5BMeSH%20Terms%5D%20AND%20%22spleen%22%5BMeSH%20Terms%5D)], (c) a perfusion agent for the heart [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxides%22%5BSubstance%20Name%5D%20AND%20%22humans%22%5BMeSH%20Terms%5D%20AND%20%28%22myocardium%22%5BMeSH%20Terms%5D%20OR%20myocardial%5BText%20Word%5D%29)], and (d) a monitoring agent for macrophage infiltration in pathological tissues [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxides%22%5BSubstance%20Name%5D%20AND%20%22humans%22%5BMeSH%20Terms%5D%20AND%20%28%22macrophages%22%5BMeSH%20Terms%5D%20OR%20macrophages%5BText%20Word%5D%29)].

## References

1. Wang, Y. X., Hussain, S. M. and Krestin, G. P. Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol11(11): 2319-31, 2001.

2. Metz, S., Bonaterra, G., Rudelius, M., Settles, M., Rummeny, E. J. and Daldrup-Link, H. E. Capacity of human monocytes to phagocytose approved iron oxide MR contrast agents in vitro. Eur Radiol14(10): 1851-8, 2004.

3. Raynal, I., Prigent, P., Peyramaure, S., Najid, A., Rebuzzi, C. and Corot, C. Macrophage endocytosis of superparamagnetic iron oxide nanoparticles: mechanisms and comparison of ferumoxides and ferumoxtran-10. Invest Radiol39(1): 56-63, 2004.

4. Weissleder, R., Elizondo, G., Josephson, L., Compton, C. C., Fretz, C. J., Stark, D. D. and Ferrucci, J. T. Experimental lymph node metastases: enhanced detection with MR lymphography. Radiology171(3): 835-9, 1989.

5. Rozenman, Y., Zou, X. M. and Kantor, H. L. Magnetic resonance imaging with superparamagnetic iron oxide particles for the detection of myocardial reperfusion. Magn Reson Imaging9(6): 933-9, 1991.

6. Litovsky, S., Madjid, M., Zarrabi, A., Casscells, S. W., Willerson, J. T. and Naghavi, M. Superparamagnetic iron oxide-based method for quantifying recruitment of monocytes to mouse atherosclerotic lesions in vivo: enhancement by tissue necrosis factor-alpha, interleukin-1beta, and interferon-gamma. Circulation107(11): 1545-9, 2003.

7. Bos, C., Delmas, Y., Desmouliere, A., Solanilla, A., Hauger, O., Grosset, C., Dubus, I., Ivanovic, Z., Rosenbaum, J., Charbord, P., Combe, C., Bulte, J. W., Moonen, C. T., Ripoche, J. and Grenier, N. In vivo MR imaging of intravascularly injected magnetically labeled mesenchymal stem cells in rat kidney and liver. Radiology233(3): 781-9, 2004.

8. Bach-Gansmo, T., Fahlvik, A. K., Ericsson, A. and Hemmingsson, A. Superparamagnetic iron oxide for liver imaging. Comparison among three different preparations. Invest Radiol29(3): 339-44, 1994.

9. Bartolozzi, C., Lencioni, R., Donati, F. and Cioni, D. Abdominal MR: liver and pancreas. Eur Radiol9(8): 1496-512, 1999.

10. Seneterre, E., Taourel, P., Bouvier, Y., Pradel, J., Van Beers, B., Daures, J. P., Pringot, J., Mathieu, D. and Bruel, J. M. Detection of hepatic metastases: ferumoxides-enhanced MR imaging versus unenhanced MR imaging and CT during arterial portography. Radiology200(3): 785-92, 1996.

11. Ros, P. R., Freeny, P. C., Harms, S. E., Seltzer, S. E., Davis, P. L., Chan, T. W., Stillman, A. E., Muroff, L. R., Runge, V. M. and Nissenbaum, M. A. Hepatic MR imaging with ferumoxides: a multicenter clinical trial of the safety and efficacy in the detection of focal hepatic lesions. Radiology196(2): 481-8, 1995.